# (1R,2S,3S,5S)-Methyl-8-{[(1S,2S)-2-([^18^F]fluoromethyl)cyclopropyl]methyl}-3-phenyl-8-azabicyclo[3.2.1]octane-2-carboxylate

Chemical name: | (1R,2S,3S,5S)-Methyl-8-{[(1S, 2S)-2-([^18^F]fluoromethyl)cyclopropyl]methyl}-3-phenyl-8-azabicyclo[3.2.1]octane-2-carboxylate
Abbreviated name: | [^18^F]PR17.MZ
Synonym:
Agent category: | Compound
Target: | Dopamine transporter (DAT)
Target category: | Transporter
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PR17.MZ)]

Dopamine, a neurotransmitter, plays an important role in the mediation of movement, cognition, and emotion. Parkinson’s disease (PD) is associated with a loss of dopamine-containing neurons in the striatum, resulting in a loss of dopamine transporter (DAT) in the presynaptic nerve terminals (1, 2). Reduction of DAT density is inversely correlated with the severity of motor dysfunction in PD patients. Several (-)-cocaine analogs were developed for the evaluation of DAT density in neurons of PD patients. Radiolabeled 2β-carboxymethoxy-3β-(4-iodophenyl)tropane (β-CIT) and N-(3-fluoropropyl)-2β-carbomethoxy-3β-(4-iodophenyl)nortropane (FP-CIT) have been used for brain imaging (3-6). Because of the short physical half-life of ^11^C-labeled analogs, equilibrium conditions are difficult to achieve in positron emission tomography (PET) measurements. [^123^I]β-CIT was studied in single-photon emission computed tomography (SPECT) and showed slow tracer uptake kinetics (7, 8). A tropane derivative, [^11^C]-(E)-N-(4-fluorobut-2-enyl)-2β-carbomethoxy-3β-(4'-tolyl)nortropane ([^11^C]LBT-999), was evaluated as a radioligand for studies of DAT with PET imaging (9-11). [1R,2S,3S,5S]-Methyl-8-{[(1S, 2S)-2-([^18^F]fluoromethyl)cyclopropyl]methyl}-3-phenyl-8-azabicyclo[3.2.1]octane-2-carboxylate ([^18^F]PR17.MZ) was developed through the use of a conformational restriction approach based on (-)-cocaine. PR17.MZ exhibited a 29-fold higher potency than (-)-cocaine in inhibition of human DAT and better selectivity over the human noradrenalin transporter (hNET) and human serotonin transporter (hSERT) (12). [^18^F]PR17.MZ has been evaluated as a radioligand for studies of DAT with PET imaging.

### Related Resource Links:

- Chapters in MICAD (DAT (http://www.ncbi.nlm.nih.gov/books?term=(DAT%20or%20dopamine%20transporter)%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (DAT (http://www.ncbi.nlm.nih.gov/gene/6531))
- Articles in Online Mendelian Inheritance in Man (OMIM) (DAT (http://www.ncbi.nlm.nih.gov/omim/126455))
- Clinical trials (DAT (http://www.clinicaltrials.gov/ct2/results?term=DAT+imaging))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PR17.MZ%20AND%20synthesis)]

[^18^F]PR17.MZ was readily synthesized by standard ^18^F-fluorination of the bromo-derivative with [^18^F]KF/Kryptofix 2.2.2 for 50 s in a focused microwave reactor (250 W, 180°C) (12). [^18^F]PR17.MZ was purified with high-performance liquid chromatography. Overall radiochemical yield (decay-corrected) was 86%, with a specific activity of 180 GBq/µmol (4.9 Ci/µmol) at the end of synthesis and a radiochemical purity of >98%. Total synthesis time was not reported.

## In Vitro studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PR17.MZ%20AND%20in%20vitro)]

PR17.MZ binding affinity for hDAT, hSERT, and hNET was determined using stably transfected HEK293 cells (12). [^3^H]β-CFT, [^3^H]citalopram, and [^3^H]nisoxetine were used as radioligands, respectively. The 50% inhibition concentration values for hDAT, hSERT, and hNET were 11 nM, 1,400 nM, and 175 nM, respectively. In vitro autoradiography studies with [^18^F]PR17.MZ in rat brain sections showed a high radioactivity level in the striatum, with low binding in the cortical regions and cerebellum. Binding in the brain was totally blocked in the presence of 1 µM β-CFT.

## Animal Studies

### Rodents

[PubMed] (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PR17.MZ%20AND%20rodentia)

Riss et al. (12) performed dynamic PR17.MZ PET brain scans of normal rats (n = 3). Striatal peak accumulation of 0.92 ± 0.06% injected dose/ml (ID/ml) was reached at 70 s after injection, followed by a gradual washout to 0.49 ± 0.06% ID/ml and 0.23 ± 0.03% ID/ml at 20 min and 45 min, respectively. The accumulation in the cerebellum was 0.32 ± 0.08% ID/ml and 0.12 ± 0.06% ID/ml at 10 s and 20 min, respectively. Co-injection of β-CFT (1.5 mg/kg) with the tracer displaced the radioactivity in the striatum to the background level at 90 min after injection. The equilibrium state between the striatum and cerebellum was reached as soon as 20 min. Logan graphical analysis provided a distribution volume ratio of ~3 for the striatum.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=PR17.MZ+AND+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PR17.MZ%20AND%20monkeys)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PR17.MZ%20AND%20human)]

No publication is currently available.

## References

1 Carbon M., Ghilardi M.F., Feigin A., Fukuda M., Silvestri G., Mentis M.J., Ghez C., Moeller J.R., Eidelberg D. (2003). Learning networks in health and Parkinson's disease: reproducibility and treatment effects. Hum Brain Mapp.
2 Chesselet M.F., Delfs J.M. (1996). Basal ganglia and movement disorders: an update. Trends Neurosci.
3 Abi-Dargham A., Gandelman M.S., DeErausquin G.A., Zea-Ponce Y., Zoghbi S.S., Baldwin R.M., Laruelle M., Charney D.S., Hoffer P.B., Neumeyer J.L., Innis R.B. (1996). SPECT imaging of dopamine transporters in human brain with iodine-123-fluoroalkyl analogs of beta-CIT. J Nucl Med.
4 Chaly T., Dhawan V., Kazumata K., Antonini A., Margouleff C., Dahl J.R., Belakhlef A., Margouleff D., Yee A., Wang S., Tamagnan G., Neumeyer J.L., Eidelberg D. (1996). Radiosynthesis of [18F] N-3-fluoropropyl-2-beta-carbomethoxy-3-beta-(4-iodophenyl) nortropane and the first human study with positron emission tomography. Nucl Med Biol.
5 Kazumata K., Dhawan V., Chaly T., Antonini A., Margouleff C., Belakhlef A., Neumeyer J., Eidelberg D. (1998). Dopamine transporter imaging with fluorine-18-FPCIT and PET. J Nucl Med.
6 Lundkvist C., Halldin C., Ginovart N., Swahn C.G., Farde L. (1997). [18F] beta-CIT-FP is superior to [11C] beta-CIT-FP for quantitation of the dopamine transporter. Nucl Med Biol.
7 Ishikawa T., Dhawan V., Kazumata K., Chaly T., Mandel F., Neumeyer J., Margouleff C., Babchyck B., Zanzi I., Eidelberg D. (1996). Comparative nigrostriatal dopaminergic imaging with iodine-123-beta CIT-FP/SPECT and fluorine-18-FDOPA/PET. J Nucl Med.
8 Laruelle M., Wallace E., Seibyl J.P., Baldwin R.M., Zea-Ponce Y., Zoghbi S.S., Neumeyer J.L., Charney D.S., Hoffer P.B., Innis R.B. (1994). Graphical, kinetic, and equilibrium analyses of in vivo [123I] beta-CIT binding to dopamine transporters in healthy human subjects. J Cereb Blood Flow Metab.
9 Chalon S., Hall H., Saba W., Garreau L., Dolle F., Halldin C., Emond P., Bottlaender M., Deloye J.B., Helfenbein J., Madelmont J.C., Bodard S., Mincheva Z., Besnard J.C., Guilloteau D. (2006). Pharmacological characterization of (E)-N-(4-fluorobut-2-enyl)-2beta-carbomethoxy-3beta-(4'-tolyl)nortropane (LBT-999) as a highly promising fluorinated ligand for the dopamine transporter. J Pharmacol Exp Ther.
10 Dolle F., Emond P., Mavel S., Demphel S., Hinnen F., Mincheva Z., Saba W., Valette H., Chalon S., Halldin C., Helfenbein J., Legaillard J., Madelmont J.C., Deloye J.B., Bottlaender M., Guilloteau D. (2006). Synthesis, radiosynthesis and in vivo preliminary evaluation of [11C]LBT-999, a selective radioligand for the visualisation of the dopamine transporter with PET. Bioorg Med Chem.
11 Saba W., Valette H., Schollhorn-Peyronneau M.A., Coulon C., Ottaviani M., Chalon S., Dolle F., Emond P., Halldin C., Helfenbein J., Madelmont J.C., Deloye J.B., Guilloteau D., Bottlaender M. (2007). [11C]LBT-999: a suitable radioligand for investigation of extra-striatal dopamine transporter with PET. Synapse.
12 Riss P.J., Piel M., Bockhart V., Bausbacher N., Buchholz H.G., Lueddens H., Roesch F. (2010). The DAT ligand [(18)F]PR17.MZ mirrors the in vivo pharmacokinetic profile of [(11)C]cocaine with significantly improved monoamine transporter selectivity. ChemMedChem.